# [^123^I]Vascular endothelial growth factor

Chemical name: | [^123^I]Vascular endothelial growth factor
Abbreviated name: | [^123^I]VEGF_165_
Synonym:
Agent Category: | Polypeptide
Target: | VEGF receptors
Target Category: | Receptor binding
Method of detection: | SPECT, planar
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms of various number of amino acids (121, 145, 165, 183, 189 and 206) produced through alternative splicing (1). VEGF_121_, VEGF_165_ and VEGF_189_ are the major forms secreted by most cell types. They are active as homodimers linked by disulfide bonds. VEGF_165_ is the best-characterized VEGF species. VEGF is a potent angiogenic factor inducing proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high affinity tyrosine kinase receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts and pancreatic beta cells also express VEGF receptors (1).

VEGF receptors were found to be overexpressed in various tumor cells and tumor-associated endothelial cells (2). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis and tumor growth and metastasis (3, 4). [^123^I]VEGF_165_ was developed as a SPECT tracer for imaging solid tumors and angiogenesis (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20synthesis)]

VEGF_165_ was labeled with sodium [^123^I]iodide by electrophilic radioiodination using the chloramine-T method (5). This method gave a radiochemical yield of >25% and a radiochemical purity of >97% in a specific activity of 42.3 mCi/nmol (1.66 GBq/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20in%20vitro)]

[^123^I]VEGF_165_ (0.001 nM) induced proliferation of human umbilical vein endothelial cells (HUVECs) and A431 mammary carcinoma cells to a similar extent as unlabeled VEGF_165_ (5). Two classes of high-affinity [^123^I]VEGF_165_-binding sites (B_max1_ = 518 sites/cell, K_d1_ = 26 pM and B_max2_ = 6,100 sites/cell, K_d2_ = 2.07 nM) were found on the cell surfaces of HUVECs. In contrast, one class of binding site (B_max_ = 1,290-3,540 sites/cell and K_d_ = 88-167 pM) was found on various human cell lines such as HMC-1 mast cells, A431 mammary carcinoma, HEP-G2 hepatoma, HEP-1 hepatic endothelioma, and U937 monocyte cells as well as many human primary tumors (5). No specific binding sites were detected in undifferentiated adenocarcinoma cells as compared with differentiated adenocarcinoma cells (B_max_ = 15.6 fmol/10^7^ cells, K_d_ = 143 pM) (6). Tumor cells expressed a significantly higher number of [^123^I]VEGF_165_ binding sites on their cell surfaces than normal blood cells and adjacent normal tissues (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20rodentia)]

Cornelissen et al. (7) performed biodistribution and imaging studies of [^123^I]VEGF_165_ in normal mice. The organs with the highest accumulation were the kidneys (30.1 ± 11.2% ID at 1.5 min), liver (14.6 ± 4.9% ID at 1.5 min) and stomach (13.2 ± 3.5% ID at 3 h). Low background activity was observed in the lungs, heart, body and head (containing the thyroid, which was not dissected separately). Bladder content radioactivity was found to be high. Background levels in the lungs and intestines were low, as shown by both biodistribution and planar gamma camera images. Biodistribution in A2058 tumor-bearing nude mice showed tumor/thigh ratios of 0.40 ± 0.14, 6.12 ± 2.11, 1.16 ± 0.30 and 0.48 ± 0.12 at 1, 2, 4 and 6 h after injection, respectively. Other organs did not differ significantly from the results obtained from normal mice. Co-injection of 80 μg of VEGF_165_ resulted in a significant decrease of the tumor/thigh from 6.01 ± 1.95 to 1.30±0.34 (P<.05) at 2 h after injection. Tumor/thigh ratio of the CAPAN-II-(VEGF receptor negative) bearing mice was 1.11±0.23.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20human)]

[^123^I]VEGF_165_ (184 ± 18 MBq, 5 ± 0.5 mCi; 0.13 nmol) was administered intravenously to 18 patients with gastrointestinal tumors (8). SPECT images with [^123^I]VEGF_165_ were compared with computed tomography (CT) and magnetic resonance imaging (MRI). Binding of [^123^I]VEGF_165_ to primary tumors and metastases was visible shortly after injection. In patients with pancreatic adenocarcinoma, primary tumors were visualized by imaging in 7 of 9, lymph node metastases in 3 of 4, liver metastases in 3 of 6 and lung metastases in 1 of 3. Cholangiocarcinomas were visualized by imaging in 1 of 2 patients. Hepatocellular carcinomas were visible by imaging in 2 of 4 patients. [^123^I]VEGF_165_ images were weakly positive in one patient with abdominal schwannoma and in 1 patient with peritoneal carcinosis. A ring-shaped tracer accumulation around the necrotic tumors was observed. [^123^I]VEGF_165_ SPECT provided an overall specificity of 58% and CT/MRI provided a specificity of 95%.

Human dosimetry of [^123^I]VEGF_165_ was determined from blood samples and SPECT images in 9 patients with pancreatic adenocarcinoma after intravenous injection of 189 ± 17 MBq (5.1 ± 0.5 mCi). [^123^I]VEGF_165_ disappeared rapidly from the blood to 4% in 30 min postinjection (6).High uptake in the lungs, liver, kidneys and spleen was observed in 30 min. There was a rapid uptake of the tracer by the primary pancreatic adenocarcinoma (tumor/background ratios, 1.3 to 2.7) within 30 min by SPECT scans. The images were still visible at 3 h. The overall sensitivity of [^123^I]VEGF_165_ scintigraphy for detecting primary pancreatic tumors and their metastases was 64% (14 of 22 lesions) visualizing primary pancreatic adenocarcinoma in 7 of 9 patients (sensitivity, 78%). The effective dose was estimated to be 0.017 mSv/MBq (63 mrem/mCi). The organ that received the highest dose was the thyroid (0.058 mGy/MBq or 0.21 rad/mCi), followed by the spleen (0.046 mGy/MBq or 0.17 rad/mCi), urinary bladder (0.040 mGy/MBq or 0.15 rad/mCi), lungs (0.034 mGy/MBq or 0.13 rad/mCi) kidneys (0.033 mGy/MBq or 0.12 rad/mCi), and liver (0.029 mGy/MBq or 0.11 rad/mCi).

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
3 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
4 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
5 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
6 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
7 Cornelissen B., Oltenfreiter R., Kersemans V., Staelens L., Frankenne F., Foidart J.M., Slegers G. (2005). In vitro and in vivo evaluation of [123I]-VEGF165 as a potential tumor marker. Nucl Med Biol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.